# ^111^In-Diethylenetriaminepentaacetic acid-Lys^40^-exendin-3

Chemical name: | ^111^In-Diethylenetriaminepentaacetic acid-Lys^40^-exendin-3
Abbreviated name: | ^111^In-DTPA-Lys^40^-exendin-3
Synonym:
Agent category: | Peptide
Target: | Glucagon-like peptide-1 receptor (GLP-1R)
Target category: | Receptor
Method of detection: | Single-photon emission computed tomography (SPECT), gamma imaging
Source of signal: | ^111^In
Activation: | No
Studies: | - In vitro; - Rodents | Structure not available in PubChem (http://pubchem.ncbi.nlm.nih.gov/).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=111In%20Exendin-3)]

Glucagon-like peptide-1 (GLP-1, 30 amino acids) is secreted from enteroendocrine cells of the distal small intestine in response to food ingestion (1). GLP-1 plays an important role in glucose metabolism and homeostasis, and it inhibits gastric emptying, glucagon secretion, and glucose production (2). In addition, GLP-1 induces insulin release from β-cells in the pancreas. GLP-1 also induced proliferation of the pancreatic β-cells. The GLP-1 receptor (GLP-1R) has been identified in normal tissues such as the pancreas, stomach, brain, and lung, and it has been shown to be highly overexpressed in human insulinomas and gastrinomas (3). In insulinomas, GLP-1R density is considerably greater, and the GLP-1R is more frequently observed than somatostatin receptors.

Exendin-4 is a GLP-1 analog with 39 amino acids isolated from the venom of the Gila monster (Heloderma suspectum) (4). Exendin-4 and GLP-1 share a 53% amino acid sequence homology. Exendin-4 is a more potent and longer-lasting GLP-1R agonist than GLP-1. Exendin-4 is resistant to cleavage by dipeptidyl peptidase IV, whereas the first two N-terminal amino acids of GLP-1 are rapidly cleaved. ^111^In-Diethylenetriamine pentaacetic acid-aminohexanoic acid-Lys^40^-exendin-4 (^111^In-DTPA-Ahx-Lys^40^-exendin-4) has been developed for single-photon emission computed tomography (SPECT) imaging of the GLP-1R (5, 6). Exendin-3 and exendin-4 differ in two amino acids (positions 2 and 3), which are located in the region of the peptide that is responsible for internalization of the ligand-receptor complex. Brom et al. (7) investigated the usefulness of DTPA-Lys^40^-exendin-3 (^111^In-DTPA-Lys^40^-exendin-3) as a SPECT agent for imaging insulinomas.

### Related Resource Links:

- Chapters in MICAD (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=books&Cmd=DetailsSearch&Term=GLP-1%5BAll+Fields%5D+AND+micad%5Bbook%5D)
- Gene information in NCBI (GLP-1R (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=gene&Cmd=DetailsSearch&Term=2740%5Buid%5D)).
- Articles in OMIM (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=omim&Cmd=DetailsSearch&Term=GLP-1)
- Clinical trials (Exendin (http://www.clinicaltrials.gov/ct2/results?term=GLP-1))
- Drug information in FDA (http://google2.fda.gov/search?q=exendin&client=FDAgov&site=FDAgov&lr=&proxystylesheet=FDAgov&output=xml_no_dtd&getfields=*&x=11&y=18)

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=111In%20Exendin-3%20and%20synthesis)]

A mixture of 150 MBq (4.1 mCi) ^111^InCl_3_ and DTPA-Lys^40^-exendin-3 was incubated in buffer (pH 5.5) for 30 min at room temperature. ^111^In-DTPA-Lys^40^-exendin-3 was identified with high-performance liquid chromatography (HPLC). ^111^In-DTPA-Lys^40^-exendin-3 exhibited a radiochemical purity of >95% and a specific activity of 700 GBq/µmol (19 Ci/µmol) after HPLC purification.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=111In%20Exendin-3%20and%20in%20vitro)]

Brom et al. (7) reported that ^nat^In-DTPA-Lys^40^-exendin-3, ^nat^In-DOTA-Lys^40^-exendin-3, and ^nat^Ga-DOTA-Lys^40^-exendin-3 exhibited 50% inhibitory concentration (IC_50_) values of 8.5 nM, 5.3 nM, and 5.7 nM, respectively. The inhibition assays were performed with GLP-1R–expressing rat insulinoma INS-1 cells and ^111^In-DTPA-Lys^40^-exendin-3. ^111^In-DTPA-Lys^40^-exendin-3 (~55 fmol) was specifically accumulated into INS-1 cells in culture with 0.5 fmol at 0.5 h and 6.5 fmol at 4 h. Most of the accumulated radioactivity was internalized into the cells (60–80%). No blocking studies were reported.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=111In%20Exendin-3%20and%20rodentia)]

Brom et al. (7) performed biodistribution studies in nude mice (n = 5) bearing INS-1 insulinomas that consisted of injection of 0.37 MBq (10 μCi) ^111^In-DTPA-Lys^40^-exendin-3 or ^111^In-DTPA-Lys^40^-exendin-4. An experiment that consisted of coinjection of excess exendin-3 was also performed. Tumor accumulation was 36.0 ± 5.5% injected dose/gram (ID/g) and 36.3 ± 8.0% ID/g at 4 h after injection of ^111^In-DTPA-Lys^40^-exendin-3 or ^111^In-DTPA-Lys^40^-exendin-4, respectively. Excess exendin-3 reduced the tumor accumulation to the background level (~1% ID/g). Specific and moderate uptake was observed in the pancreas, stomach, and lung. Uptake in the kidneys was ~140% ID/g and was not displaced by exendin-3. Marginal accumulation (<1% ID/g) was observed in the muscle, blood, heart, spleen, and liver. As a comparison, tumor accumulation of ^111^In-DTPA-Lys^40^-exendin-3 and ^111^In-DTPA-Lys^40^-exendin-4 was more than two-fold higher than that of ^68^Ga-DOTA-Lys^40^-exendin-3.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=111In%20Exendin-3%20and%20%28dog%20or%20pig%20or%20sheep%20or%20rabbit%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=111In%20Exendin-3%20and%20%28primate%20not%20human%29)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=111In%20Exendin-3%20and%20human)]

No publication is currently available.

## NIH Support

1R01 AG030328-01

## References

1 Theodorakis M.J., Carlson O., Michopoulos S., Doyle M.E., Juhaszova M., Petraki K., Egan J.M. (2006). Human duodenal enteroendocrine cells: source of both incretin peptides, GLP-1 and GIP. Am J Physiol Endocrinol Metab.
2 Doyle M.E., Egan J.M. (2001). Glucagon-like peptide-1. Recent Prog Horm Res.
3 Reubi J.C., Waser B. (2003). Concomitant expression of several peptide receptors in neuroendocrine tumours: molecular basis for in vivo multireceptor tumour targeting. Eur J Nucl Med Mol Imaging.
4 Meier J.J., Nauck M.A. (2005). Glucagon-like peptide 1(GLP-1) in biology and pathology. Diabetes Metab Res Rev.
5 Gotthardt M., Lalyko G., van Eerd-Vismale J., Keil B., Schurrat T., Hower M., Laverman P., Behr T.M., Boerman O.C., Goke B., Behe M. (2006). A new technique for in vivo imaging of specific GLP-1 binding sites: First results in small rodents. Regul Pept.
6 Wild D., Behe M., Wicki A., Storch D., Waser B., Gotthardt M., Keil B., Christofori G., Reubi J.C., Macke H.R. (2006). [Lys40(Ahx-DTPA-111In)NH2]Exendin-4, a Very Promising Ligand for Glucagon-like Peptide-1 (GLP-1) Receptor Targeting. J Nucl Med.
7 Brom M., Oyen W.J., Joosten L., Gotthardt M., Boerman O.C. (2010). 68Ga-labelled exendin-3, a new agent for the detection of insulinomas with PET. Eur J Nucl Med Mol Imaging.